# Survivin specified small interfering RNA-CLIO-Cy5.5

Chemical name: | Survivin specified small interfering RNA-CLIO-Cy5.5
Abbreviated name: | siSurvivin-CLIO-Cy5.5
Synonym: | MN-NIFR-siSurvivin
Agent category: | Nucleic acid, small molecule (nanoparticle)
Target: | RNAse III
Target category: | Enzyme
Method of detection: | Magnetic resonance imaging (MRI), near-infrared (NIFR) optical imaging
Source of signal/contrast: | Iron oxides, Cy5.5
Activation: | No
Studies: | - Rodents | No structure is Currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLIO + cy5.5 + siSurvivin)]

Ribonucleic acid interference (RNAi) modulates intracellular activation via the use of small interfering RNA (siRNA) (1). RNAi suppresses gene expression through degradation of a specific, targeted mRNA, which leads to gene silencing. siRNA is a 21-23 nucleotide (nt) double-stranded RNA (dsRNA) with symmetric 2-3nt 3’ overhangs and 5’-phosphate and 3’-hydroxyl groups so that it is recognized by an RNAse III enzyme (2). In general, intracellular siRNA undergoes 5’-phosphorylation to unwind the RNA duplex, followed by association with RNA-induced silencing complex (RISC) (1). Then the activated RISC and the unwound anti-sense strand of the siRNA interact with the mRNA target to generate single site-specific cleavage at the mRNA target. The efficiency of gene silencing primarily relies on the optimal incorporation of siRNA into RISC and its stability in RISC, as well as a perfect complementary base pairing with the mRNA target (3). Mismatches can abolish the target degradation, the mRNA cleavage, and the RISC turnover. The high specificity in gene silencing makes siRNA a popular research tool for various gene-inactivation studies such as differentiation, apoptosis, and tumorigenesis (3). siRNA is also used in therapeutic applications to identify drug targets and to characterize gene functions in vivo without the use of gene knockout mice (4). Formulation of siRNAs with compounds to promote transit across cell membranes is being developed to address the major challenge of cellular delivery of siRNAs (5). Several imaging modalities have been used for localized in vivo delivery of siRNA (6).

Survivin is a small protein (142 amino acids, 16.5 kDa) that belongs to the inhibitor of apoptosis protein (IAP) family (7). This type of protein can effectively suppress apoptosis induced by a variety of stimuli, including death receptor activation, growth factor withdrawal, ionizing radiation, viral infection, and genotoxic damage. Survivin comprises a single baculovirus IAP repeat (BIR) domain and an extended COOH-terminal α-helical coiled-coil domain but lacks the RING-finger domain found in the other IAPs. In addition to apoptosis, survivin is involved in many essential cellular functions, such as cell division, cell stress response, and surveillance checkpoints. Survivin is strongly expressed in the majority of human tumor types, including lung, breast, colon, gastric oesophageal, pancreatic, liver, bladder, uterine, and ovarian cancers, large-cell non-Hodgkins lymphomas, leukemias, neuroblastomas, brain tumors, pheochromocytomas, soft tissue sarcomas, melanomas, and other kinds of cancers (8). As a new target in cancer treatment, inhibition of survivin expression can be carried out through the use of anti-sense oligonucleotides, ribozymes, and siRNA (8). Survivin-specified siRNA (siSurvivin) is designed to target the anti-apoptotic gene Birc5 that encodes survivin (9).

siSurvivin-crosslinked iron oxide nanoparticles (CLIO)-Cy5.5 (siSurvivin-CLIO-Cy5.5) is a magnetofluorescent nanoparticle used for multimodal imaging of the delivery and silencing of siSurvivin in tumors (6). This agent consists of four components: five siSurvivins to target survivin mRNA, three fluorescence probes (Cy5.5) for optical imaging, four myristoylated polyarginine peptides (MPAP) for mediating transportation to the cytoplasm, and an iron oxide nanoparticle core for enhancing magnetic resonance imaging (MRI) contrast and delivering siSurvivin to tumors. The siSurvivin is linked to the magnetic nanoparticles by a stable thioether bond without compromising silencing efficiency. Cy5.5 is a cyanine dye consisting of two quaternized heteroaromatic bases (A and A’) joined by a polymethine chain with five carbons (10), and it is directly bound to the nanoparticles. This dye possesses high quantum yield, good chemical stability, easy conjugation, and high sensitivity (mole extinction coefficient, ~250,000 mol/cm) (11, 12). As a membrane translocation module, MPAP has a hydrophobic 14-carbon moiety of myristic acid (Myr, -C(=O)-(CH_2_)_12_-CH_3_) linked to a polyarginine peptide to generate Myr-Ala-(ARg)_7_-Cys-CONH_2_ (13). MPAP can cross the cellular membrane of live cells efficiently and target the cytoplasm without registered toxicity (13). The nanoparticle contains an icosahedral core of superparamagnetic crystalline Fe_3_O_4_ (magnetite) that is caged by epichlorohydrin cross-linked dextran and functionalized with amine groups (CLIO-NH_2_) (14). They have a high magnetic susceptibility to induce a significant magnetization inside a magnetic field. This creates microscopic field gradients that diphase nearby protons and causes a shortening of T_2_ relaxation times (15). Enhanced permeability and retention effects in tumors and an increased fluid-phase endocytosis in tumor cells result in the accumulation of magnetic nanoparticles in the tumors (6). With the assistance of MPAP, sufficient siSurvivin can be delivered to the tumors. siSurvivin-CLIO-Cy5.5 allows for fine resolution (10–100 μm) and unlimited depth penetration of MRI with the high sensitivity (10^-9^–10^-17^ mol/L) and the short acquisition times of optical imaging (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO + cy5.5 + siSurvivin)+AND+synthesis%0D%0A)]

The synthesis of siSurvivin-CLIO-Cy5.5 was conducted in multiple steps (6). Initially, monocrystalline iron oxide (MION) was synthesized by neutralization of ferrous salts, ferric salts, and dextran with ammonium hydroxide, followed by ultrafiltration (16). The obtained MION was cross-linked in strong base with epichlorohydrin and then reacted with ammonia to produce CLIO-NH_2._ Next, N-hydroxysuccinimide ester of Cy5.5 was reacted with the CLIO-NH_2_ (17). The produced CLIO-Cy5.5 was conjugated with a heterobifunctional cross-linker, N-succinimidyl 3-(2-pyridyldithio)propionate (SPDP), via N-hydroxysuccinimide ester. Then, Myr-Ala-(ARg)_7_-Cys-CONH_2_ MPAPs were attached to this linker via a sulfhydryl reactive pyridyl disulfide residue (pH 7). The produced CLIO(MPAP)-Cy5.5 was coupled with an m-maleimidobenzoyl-N-hydroxysuccinimide ester (MBS) cross-linker (pH 8.5). At the same time, a commercial siRNA duplex to human survivin was modified with a thiol moiety via a hexyl spacer (5’-S-S-(CH_2_)_6_-) for bioconjugation. Finally, the free thiol single-stranded RNA was reacted with the CLIO(MPAP)-Cy5.5 via the MBS cross-linker to produce siSurvivin-CLIO-Cy5.5. The analysis results demonstrated that on average there were three Cy5.5, four MPAP, and five siSurvivin molecules per paramagnetic nanoparticle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( CLIO + cy5.5 + siSurvivin)+AND+%22in+vitro%22)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO+ cy5.5 + siSurvivin) +AND++rodentia)]

Medarova et al. studied the in vivo effect of siSurvivin-CLIO-Cy5.5 in tumors (6). Nude mice (n = 5) were implanted with human colon adenocarcinoma LS174T cells on the right flank. The delivery of siSurvivin-CLIO-Cy5.5 was examined with MRI at 9.4 T; T_2_-weighted images were collected at 10–14 days after the inoculation, when tumors grew to ~0.5 cm in diameter. siSurvivin-CLIO-Cy5.5 was injected intravenously at a dose of 10 mg Fe/kg (440 nmol siSurvivin/kg) twice per week for 2 weeks. There was a significant drop in T_2_ relaxation times in tumors after injection of siSurvivin-CLIO-Cy5.5, which was further confirmed by near-infrared optical imaging at Cy5.5 channel. The injection of siSurvivin-CLIO-Cy5.5 did not appear to induce serum interferon-α activation. The specific silencing efficiency of siSurvivin-CLIO-Cy5.5 was examined with in vitro reverse-transcription polymerase chain reaction. The transcript levels of Survivin in the tumors treated with siSurvivin-CLIO-Cy5.5 were 97 ± 2% lower than the levels observed in the controls, which were treated with the parental magnetic nanoparticles; the levels were 83 ± 2% lower than the levels seen in mice treated with the mismatch control siRNA. Frozen sections of 7-mm-thick were used to assess the apoptosis and necrosis in tumors. The level of apoptosis was evaluated by a terminal deoxynucldotidyl transferase dUTP nick end labeling (TUNEL) assay and the level of necrosis was evaluated by hematoxylin and eosin (H&E) staining. Both apoptosis and necrosis were also much higher in the tumors than in the controls.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO+ cy5.5 + siSurvivin) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(CLIO+ cy5.5 + siSurvivin) +AND+human)]

No publication is currently available.

## References

1 Chiu Y.L., Ali A., Chu C.Y., Cao H., Rana T.M. (2004). Visualizing a correlation between siRNA localization, cellular uptake, and RNAi in living cells. Chem Biol.
2 Dykxhoorn D.M., Novina C.D., Sharp P.A. (2003). Killing the messenger: short RNAs that silence gene expression. Nat Rev Mol Cell Biol.
3 Fuchs U., Borkhardt A. (2007). The application of siRNA technology to cancer biology discovery. Adv Cancer Res.
4 Tiscornia G., Singer O., Ikawa M., Verma I.M. (2003). A general method for gene knockdown in mice by using lentiviral vectors expressing small interfering RNA. Proc Natl Acad Sci U S A.
5 Mahmood Ur R., Ali I., Husnain T., Riazuddin S. (2008). RNA interference: The story of gene silencing in plants and humans. Biotechnol Adv.
6 Medarova Z., Pham W., Farrar C., Petkova V., Moore A. (2007). In vivo imaging of siRNA delivery and silencing in tumors. Nat Med.
7 Pennati M., Folini M., Zaffaroni N. (2008). Targeting survivin in cancer therapy. Expert Opin Ther Targets.
8 Zaffaroni N., Pennati M., Daidone M.G. (2005). Survivin as a target for new anticancer interventions. J Cell Mol Med.
9 Altieri D.C. (2008). Survivin, cancer networks and pathway-directed drug discovery. Nat Rev Cancer.
10 Ernst L.A., Gupta R.K., Mujumdar R.B., Waggoner A.S. (1989). Cyanine dye labeling reagents for sulfhydryl groups. Cytometry.
11 Lin Y., Weissleder R., Tung C.H. (2002). Novel near-infrared cyanine fluorochromes: synthesis, properties, and bioconjugation. Bioconjug Chem.
12 Ballou B., Fisher G.W., Hakala T.R., Farkas D.L. (1997). Tumor detection and visualization using cyanine fluorochrome-labeled antibodies. Biotechnol Prog.
13 Pham W., Zhao B.Q., Lo E.H., Medarova Z., Rosen B., Moore A. (2005). Crossing the blood-brain barrier: a potential application of myristoylated polyarginine for in vivo neuroimaging. Neuroimage.
14 Josephson L., Perez J.M., Weissleder R. (2001). Magnetic nanosensors for the detection of oligonucleotide sequences. Angew. Chem. Int. Ed. Engl.
15 Bulte J.W., Brooks R.A., Moskowitz B.M., Bryant L.H., Frank J.A. (1998). T1 and T2 relaxometry of monocrystalline iron oxide nanoparticles (MION-46L): theory and experiment. Acad Radiol.
16 Wunderbaldinger P., Josephson L., Weissleder R. (2002). Crosslinked iron oxides (CLIO): a new platform for the development of targeted MR contrast agents. Acad Radiol.
17 Montet X., Montet-Abou K., Reynolds F., Weissleder R., Josephson L. (2006). Nanoparticle imaging of integrins on tumor cells. Neoplasia.